# ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHHHHH-EAYGWMDF-NH_2_ peptide

Chemical name: | ^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHHHHH-EAYGWMDF-NH_2_ peptide
Abbreviated name: | ^111^In-DOTA-H6-Met
Synonym: | Radiolabeled minigastrin
Agent Category: | Peptide
Target: | Gastrin/cholecystokinin-2 (CCK-2, CCK-B) receptor
Target Category: | Receptor binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=417029), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=33356159) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=887&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about.the CCK-2 receptor.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29)]

^111^In-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-HHHHHH-EAYGWMDF-NH_2_ peptide (^111^In-DOTA-H6-Met) is a radiolabeled gastrin analog that can be used for single-photon emission computed tomography (SPECT) imaging of tumors that express the gastrin/cholecystokinin-2 (CCK-2) receptor (1). ^111^In is a gamma emitter with a physical half-life (t_½_) of 2.8 days.

The gastrointestinal peptides gastrin and CCK have various regulatory functions in the brain and gastrointestinal tract (2). Gastrin and CCK have the same COOH-terminal pentapeptide amide sequence, which is the biologically active site (3). Human gastrin is a peptide composed of 34 amino acids and also exists in several C-terminal truncated forms (1). These C-terminal truncated forms include minigastrin, which is a 13-residue peptide with the sequence of LEEEEEAYGWMDF-NH_2_. CCKs exist in a variety of biologically active molecular forms that are derived from a precursor molecule comprising 115 amino acids (4). These forms range from 4 to 58 amino acids in length and include sulphated and unsulphated CCK-8, which has the structure DYMGWMDF-NH_2_. They bind to and act through transmembrane G-protein–coupled receptors (5). Two different CCK receptor subtypes have been identified in normal tissues. CCK-1 (CCK-A, alimentary) receptors have low affinity for gastrin, and CCK-2 (CCK-B, brain) receptors have high affinity for gastrin (4). They also differ in terms of molecular structure, distribution, and affinity for CCK. These receptors have also been found to be expressed or overexpressed on a multitude of tumor types (5). CCK-2 receptors have been found most frequently in medullary thyroid carcinoma, small-cell lung cancers, astrocytomas, and stromal ovarian cancers (2). CCK-1 receptors have been identified in gastroenteropancreatic tumors, meningiomas, and neuroblastoma.

Reubi et al. (6) designed a series of radiolabeled CCK-8 peptides that showed high specificity for potential in vivo imaging of tumors expressing CCK-2 receptors. de Jong et al. (7) developed an ^111^In-labeled non-sulfated CCK8 analog that used 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) as a bifunctional chelating agent. The radioligand showed high specific internalization rates in receptor-positive AR42J rat pancreatic tumor cells. von Guggenberg et al. (8) reported the synthesis of ^99m^Tc-hydrazinonicotinic acid (HYNIC)-minigastrin complexes and showed high tumor uptake in nude mice bearing AR42J tumors. Nock et al. (9) prepared ^99m^Tc-labeled minigastrin analogs and found that they displayed high specific localization in nude mice bearing AR42J tumors. Mather et al. (1) synthesized a library of different peptide sequences based on the C-terminal sequences of CCK-8 or minigastrin. These peptides were labeled with ^111^In by DOTA or diethylenetriamine pentaacetic acid (DTPA) conjugation. Although their ultimate goal was to identify an analog that could be used for radiotherapeutic applications, ^111^In-DOTA-H6-Met with a hexahistidine tag was evaluated as a potential molecular probe for CCK-2 receptors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20synthesis)]

The peptide sequence HHHHHH-EAYGWMDF-amide was obtained by solid-phase peptide synthesis under standard conditions from commercial sources (1). The N-terminus was capped with a DOTA chelating group to produce DOTA-H6-Met. The identity and purity were confirmed by matrix-assisted laser desorption/ionization mass spectroscopy and reverse-phase high-performance liquid chromatography (HPLC). Radiolabeling was performed by mixing ^111^In-chloride in ammonium acetate and 0.04-M monothioglycerol (MTG), an antioxidant, with DOTA-H6-Met in 0.01-M phosphate-buffered saline (pH 7.2). The mixture was heated at 98ºC for 15 min, and 0.1-M ethylenediamine tetraacetic acid (EDTA) was then added to quench the reaction. The labeling yield was >90%. The radiochemical purity and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20in%20vitro)]

An in vitro receptor affinity assay of ^111^In-DOTA-H6-Met was performed by using AGS human gastric tumor cells transfected with the CCK-2 receptor (AGS-CCK2R) and ^125^I-G17 as the radioligand. The inhibition constant (K_i_) and half of the maximum binding fraction (EC_50_) were 2.1 nM and 3.1 nM, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20rodentia)]

Biodistribution studies of ^111^In-DOTA-H6-Met were performed in nude mice bearing AR42J rat pancreatic tumors (1), HT29 human colorectal tumors, or CA20948 rat pancreatic tumors. Both AR42J and CA20948 tumors expressed different levels of gastrin receptors, and HT29 was a cell line transfected with a relatively low level of gastrin receptors. Each mouse received 0.2 μg of ^111^In-DOTA-H6-Met by i.v. injection. The tumor radioactivity levels at 4 h (n = 3–4), represented as percent injected dose per g (% ID/g), were 0.59 ± 0.14, 0.55 ± 0.14, and 0.26 ± 0.04 for AR42J, CA20948, and HT29 tumors, respectively. The blood radioactivity levels at 4 h were 0.20 ± 0.03, 0.21 ± 0.01, and 0.26 ± 0.03 for AR42J, CA20948, and HT29 tumors, respectively. The kidney radioactivity levels at 4 h were 2.95 ± 0.60, 3.08 ± 0.77, and 3.47 ± 0.52 for AR42J, CA20948, and HT29 tumors, respectively. No blocking study was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%28radiolabeled%20gastrin%20analogs%29%20OR%20%28111in-cck-2%20receptor%20peptide%29%29%20AND%20human)]

No publication is currently available.

## References

1 Mather S.J., McKenzie A.J., Sosabowski J.K., Morris T.M., Ellison D., Watson S.A. (2007). Selection of radiolabeled gastrin analogs for Peptide receptor-targeted radionuclide therapy. J Nucl Med.
2 Reubi J.C., Schaer J.C., Waser B. (1997). Cholecystokinin(CCK)-A and CCK-B/gastrin receptors in human tumors. Cancer Res.
3 Aly A., Shulkes A., Baldwin G.S. (2004). Gastrins, cholecystokinins and gastrointestinal cancer. Biochim Biophys Acta.
4 Wang H., Wong P.T., Spiess J., Zhu Y.Z. (2005). Cholecystokinin-2 (CCK2) receptor-mediated anxiety-like behaviors in rats. Neurosci Biobehav Rev.
5 Behr T.M., Behe M.P. (2002). Cholecystokinin-B/Gastrin receptor-targeting peptides for staging and therapy of medullary thyroid cancer and other cholecystokinin-B receptor-expressing malignancies. Semin Nucl Med.
6 Reubi J.C., Waser B. (1996). Unexpected high incidence of cholecystokinin-B/gastrin receptors in human medullary thyroid carcinomas. Int J Cancer.
7 de Jong M., Bakker W.H., Bernard B.F., Valkema R., Kwekkeboom D.J., Reubi J.C., Srinivasan A., Schmidt M., Krenning E.P. (1999). Preclinical and initial clinical evaluation of 111In-labeled nonsulfated CCK8 analog: a peptide for CCK-B receptor-targeted scintigraphy and radionuclide therapy. J Nucl Med.
8 von Guggenberg E., Behe M., Behr T.M., Saurer M., Seppi T., Decristoforo C. (2004). 99mTc-labeling and in vitro and in vivo evaluation of HYNIC- and (Nalpha-His)acetic acid-modified [D-Glu1]-minigastrin. Bioconjug Chem.
9 Nock B.A., Maina T., Behe M., Nikolopoulou A., Gotthardt M., Schmitt J.S., Behr T.M., Macke H.R. (2005). CCK-2/gastrin receptor-targeted tumor imaging with (99m)Tc-labeled minigastrin analogs. J Nucl Med.